# ^99m^Tc-Mercaptoacetyl-Gly-Gly-Gly-Affibody Z_HER2:342_

Chemical name: | ^99m^Tc-Mercaptoacetyl-Gly-Gly-Gly-Affibody Z_HER2:342_
Abbreviated name: | ^99m^Tc-MAG3-Z_HER2:342_
Synonym:
Agent category: | Antibody fragment, Affibody
Target: | EGF HER2 receptor
Target category: | Receptor
Method of detection: | SPECT, gamma planar
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1956) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20)]

Epidermal growth factor (EGF) is a cytokine that comprises 53 amino acids (6.2 kDa) and is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors: EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 and HER2 are overexpressed on many solid tumor cells such as breast, non-small cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). Trastuzumab is approved for clinical use for anti-cancer therapies in both Europe and North America. ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab -F(ab')_2_ have been developed for imaging human breast cancer (12-16). However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab´)_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2 based on the Z-domain residues (58 amino acids) from one of the IgG-binding domains of staphylococcal protein A was constructed (17). Affibody molecules exhibit high binding affinity (K_d_) to HER2 with K_d_ values <100 pM. Various radiolabeled Affibody molecules have been studied in terms of their ability to image HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. Mercaptoacetyl-Gly-Gly-Gly (MAG3) was used as a chelating linker to couple ^99m^Tc to Z_HER2:342_ Affibody (^99m^Tc-MAG3-Z_HER2:342_) (18). ^99m^Tc-MAG3-Z_HER2:342_ has been evaluated in nude mice bearing human colon adenocarcinoma tumors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20synthesis)]

MAG3-Z_HER2:342_ Affibody was prepared by standard solid-phase peptide synthesis (18). ^99m^Tc as pertechnetate was added to a solution of MAG3-Z_HER2:342_ containing Na/K tartrate and SnCl_2_. The mixture was incubated for 60 min at room temperature. The labeling efficiency of ^99m^Tc incorporation was 82 ± 12% (n = 15) with >98% purity. ^99m^Tc-MAG3-Z_HER2:342_ was purified with size-exclusion chromatography. Specific activities of the preparations were not reported. ^99m^Tc-MAG3-Z_HER2:342_ was found to be stable after incubation for 1 h in murine blood serum at 37°C or in solution containing 300-fold excess cysteine.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20in%20vitro)]

Engfeldt et al. (18) performed binding experiments with MAG3-Z_HER2:342_ with the use of a Biacore sensor chip immobilized with extracellular domain of HER2 protein. The K_d_ value of MAG3-Z_HER2:342_ was calculated to be 200 pM; the K_d_ value of Z_HER2:342_ was 80 pM. Hence, the binding affinity of the synthetic Affibody molecule MAG3-Z_HER2:342_ was 1.5-fold lower than the parent Affibody molecule Z_HER2:342_. In vitro binding specificity tests showed that binding of ^99m^Tc-MAG3-Z_HER2:342_ to SKOV-3 cells expressing HER2 was mediated by the receptors because saturation of receptors by preincubation with non-labeled Z_HER2:342_ significantly decreased binding of ^99m^Tc-MAG3-Z_HER2:342_. The antigen-binding capacity of ^99m^Tc-MAG3-Z_HER2:342_ was 86%. The cell-bound radioactivity remained at 60–80% of the initially bound activity for up to 24 h when the cells were incubated with ^99m^Tc-MAG3-Z_HER2:342_. In contrast, cells incubated with ^125^I-labeled Z_HER2:342_ retained ~35% of the original cell-associated radioactivity at 24 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20rodentia)]

Engfeldt et al. (18) performed biodistribution studies of ^99m^Tc-MAG3-Z_HER2:342_ (0.1 MBq (2.7 μCi)) in nude mice (n = 16) bearing LS174T xenografts. Each mouse was administered 0.14 nmol ^99m^Tc-MAG3-Z_HER2:342_ by subcutaneous injection. The initial tracer accumulation in the LS174T tumors was ~7% injected dose per gram (ID/g) at 1 h and remained constant at 2, 4, and 6 h after injection. The radioactivity level in tumors at 2 h was higher than in other organs and tissues at 2 h with the exception of the kidneys (~12% ID/g). Blood levels were ~0.8% ID/g at 2 h and <0.2% ID/g at 4 h. The biodistribution was characterized by quick clearance of radioactivity from blood and all organs and tissues (the radioactivity level of the intestine was not measured in this experiment). Tumor/blood ratios were 12.5, 23.8, and 39.3 at 2, 4, and 6 h after injection, respectively. Pre-administration of 83 nmol Z_HER2:342_ decreased tumor accumulation from 6.12 ± 2.02% ID/g to 0.28 ± 0.05% ID/g (P = 0.001) at 4 h after injection. Biodistribution studies were also performed in normal nude mice (n = 3) without tumors at 4 h after injection. The results showed low accumulation in all organs and tissues with the exception of the intestines (30% ID/g) and the kidneys (6% ID/g). Single-photon emission computed tomography analysis was performed in nude mice (n = 3) bearing the LS174T tumors after intravenous injection of 3 MBq (81 μCi) ^99m^Tc-MAG3-Z_HER2:342_. Tumors were clearly visualized at 6 h along with the kidneys and caecum. However, only the tumors and kidneys were visualized at 24 h. In mice pretreated with Z_HER2:342_, the tumors could not be visualized with ^99m^Tc-MAG3-Z_HER2:342_.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HER2%20342%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Engfeldt, T., A. Orlova, T. Tran, A. Bruskin, C. Widstrom, A.E. Karlstrom, and V. Tolmachev, Imaging of HER2-expressing tumours using a synthetic Affibody molecule containing the (99m)Tc-chelating mercaptoacetyl-glycyl-glycyl-glycyl (MAG3) sequence. Eur J Nucl Med Mol Imaging, 2006